# Cy5.5-Endostatin

Chemical name: | Cy5.5-Endostatin
Abbreviated name:
Synonym:
Agent category: | Polypeptide
Target: | Endostatin receptors
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71981419), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_059957.3) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=80781) for more information about endostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20endostatin)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive alternative to radionuclide imaging in small animals or with probes in close proximity of the target in humans (4, 5). Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment. It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumor cells and endoscopic imaging of the pancreas and colon.

Tumor angiogenesis represents a continuous and important process in tumor development in which the tumor attempts to gain an independent blood supply (6). This process is driven by the tumor's chronic overproduction of angiogenic factors, which bind to receptors on nearby vessel endothelial cells. Angiogenesis is essential for the growth of solid tumors and their metastases. Imaging angiogenesis may be useful for monitoring angogeneic treatments of tumors and cardiovascular diseases (7-9). Endostatin was discovered as an endogenous inhibitor of tumor angiogenesis and endothelial-cell growth (10). It is one of the most promising anti-angiogenic cancer drugs. It has been successfully coupled with Cy5.5 NIR dye for optical imaging of endostatin receptor density in tumors in mice (11, 12).

### Related Resource Links:

- Chapters in MICAD (Endostatin (http://www.ncbi.nlm.nih.gov/books?term=Endostatin%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Endostain (http://www.ncbi.nlm.nih.gov/gene/80781))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Endostatin (http://www.ncbi.nlm.nih.gov/omim/120328))
- Clinical trials (Endostatin (http://www.clinicaltrials.gov/ct2/results?term=endostatin))
- Drug information in FDA (Endostatin (http://google2.fda.gov/search?q=endostatin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=0&y=0))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20endostatin%20and%20synthesis)]

Cy5.5 monofunctional N-hydroxysuccinimide (NHS) ester was used to conjugate endostatin to form Cy5.5-endostatin, which was purified by gel filtration chromatography (12). Cy5.5-endostatin was adjusted to a final concentration of 1 mg/ml. A molar ratio of Cy5.5 to endostatin was estimated to be 1.0.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20endostatin%20and%20in%20vitro)]

Histoimmunostaining of endostatin and platelet/endothelial cell adhesion molecule 1 (PECAM-1) were performed on tissue sections from tumors (Lewis lung carcinoma, LLC), heart, and muscle of untreated mice bearing the LLC tumors (11). The pattern of endostatin staining of microvasculature revealed endostatin binding to the endothelial cells with no binding to the tumor cells. Staining of PECAM-1, specific for endothelial cells, coincided with endostatin staining on the endothelial cells. There was no detectable endostatin binding in either the skeletal muscle or heart muscle sections. These results suggest that tumor cells induced formation of new blood vessels, which processed receptors for endostatin.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20endostatin%20and%20rodentia)]

Cy5.5-endostatin (100 μg/mouse) was injected intraperitoneally (i.p.) to mice bearing a 350 mm^2^ LLC tumor in their right hind limbs (12). NIR fluorescence signal in the tumors were detected at 18, 42, 66 and 114 h after injection, with a peak at 42 h. No signal was observed at 1 h with a faint signal at 6 h. There were fewer signals from tumors with 10 or 50 μg/mouse of Cy5.5-endostatin at 42 h after i.p. injection. Four sets of control mice were established: 1. Mice containing green fluorescent protein (GFP) under the control of an actin promoter; 2. Tumor-free mice injected with endostatin-Cy5.5; 3. Mice with tumors alone; 4. Mice with tumors injected with dye alone. In all control mice, no NIR signals were detected at 1 or 5 d. Pretreatment with unlabeled endostatin (500 μg/mouse) 30 min prior to injection of 100 μg/mouse Cy5.5-endostatin completely blocked the signals from the tumors, suggesting there is a putative receptor for endostatin in vivo (11). Cy5.5-endostatin (20 mg/kg) injected intravenously to mice bearing LLC tumors showed a faster kinetics of signal onset with maximal intensity at 3 h. There was a gradual loss of intensity by 24 h and the signal remained detectable up to 72 h. These results indicate that Cy5.5-endostatin can be used for optical detection of tumor angiogenesis.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20endostatin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20endostatin%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20endostatin%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Frangioni J.V., Kim S.W., Ohnishi S., Kim S., Bawendi M.G. (2007). Sentinel Lymph Node Mapping With Type-II Quantum Dots. Methods Mol Biol.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Folkman J. (1995). Angiogenesis in cancer, vascular, rheumatoid and other disease. Nat Med.
7 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
8 Carmeliet P. (2004). Manipulating angiogenesis in medicine. J Intern Med.
9 Miller J.C., Pien H.H., Sahani D., Sorensen A.G., Thrall J.H. (2005). Imaging angiogenesis: applications and potential for drug development. J Natl Cancer Inst.
10 O'Reilly M.S., Boehm T., Shing Y., Fukai N., Vasios G., Lane W.S., Flynn E., Birkhead J.R., Olsen B.R., Folkman J. (1997). Endostatin: an endogenous inhibitor of angiogenesis and tumor growth. Cell.
11 Citrin D., Lee A.K., Scott T., Sproull M., Menard C., Tofilon P.J., Camphausen K. (2004). In vivo tumor imaging in mice with near-infrared labeled endostatin. Mol Cancer Ther.
12 Citrin D., Scott T., Sproull M., Menard C., Tofilon P.J., Camphausen K. (2004). In vivo tumor imaging using a near-infrared-labeled endostatin molecule. Int J Radiat Oncol Biol Phys.